# Cy7-Polyethylene glycol-cinnamoyl-Phe-D-Leu-Phe-D-Leu-Phe-Lys-NH_2_

Chemical name: | Cy7-Polyethylene glycol-cinnamoyl-Phe-D-Leu-Phe-D-Leu-Phe-Lys-NH_2_
Abbreviated name: | Cy7-PEG-cFlFlFK
Synonym:
Agent category: | Peptide
Target: | Formyl peptide receptor type 1 (FPR1)
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal/contrast: | Cy7
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK)]

The formyl peptide receptor (FPR) family consists of three receptor subtypes (FPR1–FPR3) (1). These G-protein–coupled receptors are found on leukocytes. FPR1 is highly expressed on neutrophils under inflammatory conditions for their emigration to the sites of injury and infection (2). However, collateral damage may occur, which can cause pain, edema, fever, and swelling. The peptide antagonist cinnamoyl-Phe-D-Leu-Phe-D-Leu-Phe-Lys-NH_2_ (cFlFlFK) specifically binds FPR1 on neutrophils (3). The peptide was conjugated with Gd-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid to the ε-amino group of Lys to form Gd-DOTA-cFlFlFK for use with MRI imaging of neutrophils at the sites of inflammation (4). Xiao et al. (5, 6) conjugated polyethylene glycol (PEG) to the ε-amino group and Cy7 to the N-terminal amino group of Lys as Cy7-PEG-cFlFlFK for use with near-infrared fluorescence (NIR) imaging of inflammation.

### Related Resource Links:

- Chapters in MICAD (cFlFlFK (http://www.ncbi.nlm.nih.gov/books/?term=cFlFlFK+AND+micad%5Bbook%5D))
- Gene information in NCBI (FPR1 (http://www.ncbi.nlm.nih.gov/gene/2357))
- Articles in Online Mendelian Inheritance in Man (OMIM) (FPR1 (http://www.ncbi.nlm.nih.gov/omim/136537))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+synthesis)]

The PEG_76_ motif (3.6 kDa) was conjugated to the ε-amino group of Lys in cFlFlFK using tert-Boc-PEG_76_-N-hydroxysuccinimide (NHS) in aqueous solution to form cFlFlFK-PEG with 80%–85% yield, and its molecular weight was confirmed with mass spectroscopy (5). PEG-cFlFlFK was incubated with Cy7-NHS ester in 1:1 molar ratio in sodium borate buffer (pH 8.5) for 2 h at 4°C, with 60% yield. Cy7-PEG-cFlFlFK (one Cy7 moiety per conjugate) was purified with high-performance liquid chromatography (>95% purity), and its molecular weight was confirmed with mass spectroscopy. Cy7-PEG-cLFFFLK (scrambled peptide) was prepared similarly as a control.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+in+vitro)]

Cy7-PEG-cFlFlFK and Cy7-PEG-cLFFFLK exhibited emission maximum wavelengths of 773–774 nm in phosphate-buffered saline (pH 7.45) at an excitation wavelength of 740 nm (5). Both Cy7 conjugates were >95% intact in 50% fetal bovine serum after 24 h at 37°C. Cy7-PEG-cFlFlFK and Cy7-PEG-cLFFFLK exhibited log P values of −1.13 ± 0.01 and −1.02 ± 0.10, respectively. The binding characteristics of Cy7-PEG-cFlFlFK to FPR1 were not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+rodentia)]

Xiao et al. (6) performed in vivo optical imaging studies in mice with phorbol myristate acetate–induced edema (inflammation) in the left ears (n = 5–6/group) after intravenous injection of Cy7-PEG-cFlFlFK or Cy7-PEG-cLFFFLK (2 nmol/mouse). Whole-body optical imaging scans were performed at 1, 2, 3, 6, and 24 h after injection. Fluorescence intensity of Cy7-PEG-cFlFlFK in the inflamed left ear reached a maximal level (2.2 × 10^8^ photons/s/cm^2^/sr) at 3 h, declined quickly by 6 h (1.6 × 10^8^ photons/s/cm^2^/sr), and then decreased slowly until 24 h (1.4 × 10^8^ photons/s/cm^2^/sr). The fluorescence signal in the right ear was 2.4-fold lower than that of the left inflamed ear and showed a continuous loss of signal. The left ear/right ear ratio at 3 h was 3.4. Cy7-PEG-cLFFFLK exhibited a similar pattern of fluorescence intensity in the left ear but at lower levels, with the maximal level (1.0 × 10^8^ photons/s/cm^2^/sr) at 3 h. The fluorescence intensity of Cy7-PEG-cLFFFLK in the right ear was similar to that in the inflamed left ear, but with continuous loss of fluorescence intensity. Pretreatment with 100 nmol PEG-cFlFlFK before Cy7-PEG-cFlFlFK injection reduced the left ear/right ear ratio at 3 h to 1.9.

Ex vivo biodistribution of Cy7-PEG-cFlFlFK was performed at 24 h after injection (6). The inflamed left ear exhibited a fluorescence level (5.2 × 10^8^ photons/s/cm^2^/sr) higher than that of the contralateral right ear (1.5 × 10^8^ photons/s/cm^2^/sr). The organs with the highest accumulation were the kidneys (10 × 10^8^ photons/s/cm^2^/sr) and liver (8.5 × 10^8^ photons/s/cm^2^/sr). The other tissues studied (the heart, lung, spleen, stomach, small intestine, muscle, and bone) exhibited fluorescence levels (<2.0 × 10^8^ photons/s/cm^2^/sr) lower than those of the inflamed left ear. Immunohistochemical staining and fluorescence microscopy confirmed the presence of neutrophils in the inflamed left ear but not in the contralateral right ear at 3 h after injection of Cy7-PEG-cFlFlFK.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cFLFLFK+human)]

No publication is currently available.

## References

1 Ye R.D., Boulay F., Wang J.M., Dahlgren C., Gerard C., Parmentier M., Serhan C.N., Murphy P.M. (2009). International Union of Basic and Clinical Pharmacology. LXXIII. Nomenclature for the formyl peptide receptor (FPR) family. Pharmacol Rev.
2 Loitto V.M., Rasmusson B., Magnusson K.E. (2001). Assessment of neutrophil N-formyl peptide receptors by using antibodies and fluorescent peptides. J Leukoc Biol.
3 Gavins F.N. (2010). Are formyl peptide receptors novel targets for therapeutic intervention in ischaemia-reperfusion injury?. Trends Pharmacol Sci.
4 Stasiuk G.J., Smith H., Wylezinska-Arridge M., Tremoleda J.L., Trigg W., Luthra S.K., Morisson Iveson V., Gavins F.N., Long N.J. (2013). Gd3+ cFLFLFK conjugate for MRI: a targeted contrast agent for FPR1 in inflammation. Chem Commun (Camb).
5 Xiao L., Zhang Y., Liu Z., Yang M., Pu L., Pan D. (2010). Synthesis of the Cyanine 7 labeled neutrophil-specific agents for noninvasive near infrared fluorescence imaging. Bioorg Med Chem Lett.
6 Xiao L., Zhang Y., Berr S.S., Chordia M.D., Pramoonjago P., Pu L., Pan D. (2012). A novel near-infrared fluorescence imaging probe for in vivo neutrophil tracking. Mol Imaging.